# ^64^Cu-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu

Chemical name: | ^64^Cu-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu
Abbreviated name: | ^64^Cu-CB-TE2A-(GSG)-KCCYSL
Synonym:
Agent category: | Peptide
Target: | Epidermal growth factor receptor-2 (EGFR-2, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa), and it is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A setapeptide sequence consisting of Lys-Cys-Cys-Tyr-Ser-Leu (KCCYSL) was identified using phage display screening to bind specifically to the extracellular domain of HER2 (17). ^111^In-1,4,7,10-tetraazacyclododecane-1,4,7-tris-acetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu (^111^In-DOTA-(GSG)-KCCYSL (http://www.ncbi.nlm.nih.gov/books/NBK23014/)) was evaluated in nude mice bearing human breast tumor xenografts for single-photon emission computed tomography imaging (18). For positron emission tomography (PET), Kumar et al. (19) prepared ^64^Cu-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu (^64^Cu-CB-TE2A-(GSG)-KCCYSL) for imaging of HER2 expression in breast tumors.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20synthesis)]

GSG-KCCYSL peptides were prepared with solid phase peptide synthesis (19). The metal chelator DOTA was coupled to the amino terminus of GSG-KCCYSL in solid phase synthesis. CB-TE2A-(GSG)-KCCYSL was purified with high-performance liquid chromatography (HPLC). The chemical purity of CB-TE2A-(GSG)-KCCYSL was 98%. CB-TE2A-(GSG)-KCCYSL (38.5 nmol) was mixed with 29.6 MBq (0.80 mCi) ^64^Cu in ammonium acetate (pH 7.0) and incubated for 90 min at 85°C. ^64^Cu-CB-TE2A-(GSG)-KCCYSL was purified with HPLC with >98% radiochemical purity and 45% labeling yield. The specific activity of ^64^Cu-CB-TE2A-(GSG)-KCCYSL was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20in%20vitro)]

Kumar et al. (19) performed in vitro binding assays of ^64^Cu-CB-TE2A-(GSG)-KCCYSL binding to human MDA-MB-435 breast carcinoma cells that express HER2 receptors. ^nat^Cu-CB-TE2A-(GSG)-KCCYSL exhibited a IC_50_ value of 31 ± 8 nM (n = 3). ^64^Cu-CB-TE2A-(GSG)-KCCYSL accumulated in MDA-MB-435 cells in a time-dependent manner at 37°C with a plateau at 45 min, whereas little radioactivity was observed in normal human mammary epithelial cells (184A1) that express low level of HER2 receptors. ^64^Cu-CB-TE2A-(GSG)-KCCYSL was stable in mouse serum at 37°C after up to 2 h of incubation with some degradation at 4-24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20rodentia)]

Kumar et al. (19) performed ex vivo biodistribution studies with 0.185 MBq (5 μCi) ^64^Cu-CB-TE2A-(GSG)-KCCYSL in SCID mice (n = 3/group) bearing MDA-MB-435 xenografts at 0.5, 1, 2, and 4 h after injection. The tumor accumulation of radioactivity at 0.5 h after injection was 0.98 ± 0.31% injected dose/gram (ID/g) and decreased to 0.17 ± 0.05% ID/g at 4 h. High accumulation levels were observed in the kidneys (6.43 ± 1.56% ID/g), liver (0.45 ± 0.05% ID/g), and lung (0.24 ± 0.02% ID/g) at 2 h after injection. The tumor/blood, tumor/muscle, and tumor/liver ratios were 6.4, 10.7, and 0.7 at 2 h after injection, respectively. Pretreatment (10 min) with ^nat^Cu-CB-TE2A-(GSG)-KCCYSL (76 nmol/mouse) inhibited the tumor radioactivity by 50% at 2 h after injection. Little inhibition was observed in the normal tissues. In comparison, ^64^Cu-CB-TE2A-(GSG)-KCCYSL exhibited lower retention in the liver and higher tumor/nontarget tissue ratios than ^64^Cu-DO3A-(GSG)-KCCYSL, which exhibited liver accumulation of 1.68 ± 0.42% ID/g and tumor/blood, tumor/muscle, and tumor/liver ratios of 2.7, 9.0, and 0.3 at 2 h after injection, respectively.

PET analysis was performed in SCID mice (the number of mice was not reported) bearing the MDA-MB-435 tumors at 2 h after injection of 12 MBq (0.32 mCi) Cu-CB-TE2A-(GSG)-KCCYSL (19). The tumors were clearly visualized along with the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20human)]

No publication is currently available.

## NIH support

P50 CA103130-01, IR21 CA137239-01A1, 2 R01 CA093375

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Karasseva N.G., Glinsky V.V., Chen N.X., Komatireddy R., Quinn T.P. (2002). Identification and characterization of peptides that bind human ErbB-2 selected from a bacteriophage display library. J Protein Chem.
18 Deutscher S.L., Figueroa S.D., Kumar S.R. (2009). In-labeled KCCYSL peptide as an imaging probe for ErbB-2-expressing ovarian carcinomas. J Labelled Comp Radiopharm.
19 Kumar S.R., Gallazzi F.A., Ferdani R., Anderson C.J., Quinn T.P., Deutscher S.L. (2010). In vitro and in vivo evaluation of Cu-radiolabeled KCCYSL peptides for targeting epidermal growth factor receptor-2 in breast carcinomas. Cancer Biother Radiopharm.